# Citrate-coated (184^th^ variant) very small superparamagnetic iron oxide particles

Chemical name: | Citrate-coated (184^th^ variant) very small superparamagnetic iron oxide particles
Abbreviated name: | VSOP-C184
Synonym:
Agent Category: | Iron oxide
Target: | Non-targeted
Target Category: | Phagocytosis
Method of detection: | Magnetic resonance imaging (MRI), magnetic resonance angiography (MRA)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

Superparamagnetic iron oxide (SPIO) particles are potent and versatile contrast media for magnetic resonance imaging (MRI), and their efficacy has been shown to increase as their diameter decreases (1) SPIO particles were originally developed as liver MRI contrast agents to improve tumor detection at T_2_-weighted imaging. Nevertheless, SPIO particles administered as a bolus (e.g., ferucarbotran (2)) only produce moderate signal enhancement, especially in the early stage of a dynamic T_1_-weighted MRI. Ultrasmall superparamagnetic iron oxide particles (USPIO), such as ferumoxtran-10 (3), can only be administered as an infusion. Current SPIO and USPIO particles present very limited benefits compared with the low-molecular weight gadolinium-based contrast media (4, 5), which acquire their blood pool effect by binding to plasma proteins after intravenous injection.

VSOP-C184, a citrate-coated very small iron oxide paramagnetic particle (VSOP) with a T_1_/T_2_ ratio higher than most SPIO and USPIO particles studied so far (e.g., NC 100150 (6) and SHU 555 C (7)), is being investigated as a novel contrast medium for magnetic resonance angiography (MRA). First results from preclinical and phase I studies have been reported in the literature (8, 9).

VSOP-C184 is the 184th variant of 200 synthesized particles in the optimization process of the core size and citrate coating, which is designed to achieve a minimum ratio of the relaxivities R_1_ and R_2_ while maximizing the blood half-life of the contrast medium. The respective values for R_1_ and R_2_ (at 0.94 T) reported by Wagner et al. (8) are 20.1 l/mmol.sec and 37.1 l/mmol.sec, respectively. VSOP-C184 has a core diameter of 4 nm and a hydrodynamic diameter of 7.0 ± 0.15 nm. Contrary to ultra SPIO particles (USPIO), which are stabilized sterically, VSOP particles are stabilized electrostatically by a complex binding mechanism between citrate and the surface of the iron particles (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%20and%20%28preparation%20OR%20synthesis%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

VSOP-C184 consists of an aqueous solution of superparamagnetic iron oxide particles (core diameter of 4 nm) coated with a citrate layer. Taupitz et al. (9) reported a total diameter of the particles of 7.0 ± 0.15 nm. The concentration of the active substance used by the authors was 29 g (0.52 mol) Fe/l. The solution also contained citric acid at a concentration of 4.16 g/l and mannitol at 60 g/l (8).

Details about the manufacturing process for coating iron oxide particles (overall size of 8.6 mm) with monomeric material were previously reported by Pilgrimm et al. (10). The values for R_1_ and R_2_ (determined in demineralized water at 0.94 T) reported by Wagner et al. (8) were 20.1 l/mmol.sec and 37.1 l/mmol.sec respectively. VSOP-C184 has an osmolality of 376 mOsm/kg H_2_O and a pH of 7.0. At room temperature, VSOP-C184 has so far proved to be stable for six months (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%20AND%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%20AND%20rodentia%5BmeSH%5D)]

Rodent studies were performed by Wagner et al. (8) on six male Wistar rats (85 days old, ≈420 g each) with VSOP-C184 at 0.015, 0.045, and 0.075 mmol Fe/kg. After intravenous injection, MRI was performed for 30 min (seven acquisitions) using a 3D gradient-echo sequence. Signal intensities were measured for selected regions of interest (ROIs) by collecting signal values inside the target tissue (of the ROI) and outside the body, without inclusion of motion artifacts (noise). Results showed that the rats exhibited a pronounced and long-lasting increase in vessel signal-to-noise ratio SNR_blood_ for all Fe concentrations. Compared with mean non-enhanced values, the mean SNR_blood_ values for the three tested doses were higher by a factor of 5.8, 10.9, and 11.4 at 2 min post-contrast. At 26 min post-contrast, mean values remained higher by a factor of 3.9, 8.8, and 9.3, respectively. This allowed excellent visualization of the thoracic and abdominal vasculature in rats, even at the lowest concentration of 0.015 mmol Fe/kg. The plasma elimination half-life of VSOP-C184 observed at 0.045 mmol Fe/kg was 21.3 ± 5.5 min.

Pharmacokinetic data were obtained by quantitatively measuring iron in the liver, spleen, and carcass, and by determining the signal intensity (SI) of liver and spleen 24 hours and 28 days after injection (for all three doses in Fe). Results showed that the T_1_ relaxation time of plasma (a critical parameter for the angiographic effect in MRI) was reduced to below 100 ms for up to 20 min post-injection of VSOP-C184 at 45 µmol Fe/kg, and for ≈40 min at 75 µmol Fe/kg (8).

Toxicity studies were performed by Wagner et al. (8) using mice and rats administered with a single bolus injection of VSOP-C184 at the following dose levels: 0.83, 1,79, 3.85, 8.3, and 17.9 mmol Fe/kg. The animals were inspected before injection and immediately, 5, 15, 30, 60 min, 3, 6, and 24 hours after injection, and the median lethal dose (“lethal dose, 50%” or LD_50_) was calculated by regression analysis (using the mortality rates at 24 h and 14 days). Results showed that the acute tolerance of VSOP-C184 was similar to that of polymer-coated SPIO and USPIO particles (11, 12). An LD_50_ in mice >17.9 mmol Fe/kg was determined for VSOP-C184, exceeding the maximum dose to be applied in humans during an examination (0.075 mmol Fe/kg) by a factor of at least 230. The LD_50_ determined in rats showed a high safety factor of at least 116.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Schnorr et al. (13) investigated the suitability of VSOP-C184 for first-pass MRA using three male mini pigs (≈6 months old, weight 16.75–20 kg), injected with VSOP-C184 at doses of 0.015, 0.025, or 0.035 mmol Fe/kg. Comparison was also made with the low-molecular weight contrast medium gadopentetate dimeglumine (Gd-DTPA) at concentrations of 0.1 and 0.2 mmol Gd/kg. Results showed that the differences between VSOP-C184 and Gd-DTPA were statistically not significant (p > or = .05), and that image quality, contrast, and delineation of vessels with VSOP-C184 at doses of 0.025 and 0.035 mmol Fe/kg were similar to those of Gd-DTPA at 0.1 and 0.2 mmol Gd/kg. The following signal enhancement values were obtained with VSOP-C184 for 0.015, 0.025, or 0.035 mmol Fe/kg: 9.4 ± 2.6; 12.31 ± 1.2; 16.53 ± 1.7 (aorta); 7.6 ± 2.2; 9.9 ± 1.0; 13.2 ± 0.5 (renal arteries). Vessel edge definition values were as follows for the three doses of VSOP-C184 were: 106.3 ± 31.0; 135.3 ± 58.8; 141.3 ± 71.0 (aorta); 102.2 ± 24.3; 146.8 ± 63.0; 126.9 ± 37.6 (renal arteries).

Other pig studies performed by Wagner et al. (8) showed that the plasma elimination half-life of VSOP-C184 (at 0.045 mmol Fe/kg) was 36.1 ± 4.2 minutes, resulting in a T_1_ relaxation time <100 ms for 30 min in the animals. The particles were shown to be mostly cleared by the liver. MRA of VSOP-C184 at a dose of 0.045 mmol Fe/kg showed an excellent depiction of the coronary arteries.

Schnorr et al. (14) performed MRI studies using VSOP-C184 on 20 rabbits (5 for each contrast agent and dose) bearing liver tumors (VX-2 carcinoma) imaged at 1.5 T. Results showed that VSOP-C184 administered at 0.015 mmol Fe/kg produced high contrast in delayed imaging, similar to the contrast observed with ferucarbotan at identical dose. Like ferucarbotran, VSOP-C184 appeared to be taken up by liver Kupffer cells, while tumors remained unaffected. Although VSOP-C184 exhibited a much longer blood half-life in humans (≈35 min for 0.015 mmol Fe/kg (9)), experiments performed by Schnorr et al. (14) showed that, similarly to ferucarbotran, VSOP-C184 produced a signal decrease reaching noise levels as early as 5 min after intravenous injection when used in combination with a moderately T_2_-weighted sequence. Schnorr et al. (14) suggested that the amount of VSOP-C184 accumulated in the liver during that time produced a sharp T_2_-shortening effect after it was phagocytosed.

At T_1_-weighted dynamic MRI, VSOP-C184 with 0.015 mmol and 0.025 mmol Fe/kg, Gd-DTPA, and ferucarbotran, the median peak contrast-to-noise ratio (CNR) values were 20.7 (25th percentile, 16.3; 75th percentile, 22.6), 24.2 (25th percentile, 19.3; 75th percentile, 28.5), 16.4 (25th percentile, 13.7; 75th percentile, 20.3), and 14.0 (25th percentile, 11.4; 75th percentile, 16.8), respectively. At T_2_-weighted imaging using the same contrast agents and same concentrations, the measured median CNR values were 15.0 (25th percentile, 13.4; 75th percentile, 21.3), 15.7 (25th percentile, 14.5; 75th percentile, 19.8), 11.3 (25th percentile, 8.2; 75th percentile, 12.2), and 15.7 (25th percentile, 12.5; 75th percentile, 22.4), respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%20AND%20%28primates%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VSOP-C184%20AND%20human)]

Taupitz et al. (9) performed phase I clinical studies of VSOP-C184 on 18 healthy male subjects (19–43 years old) at concentrations of 0.015, 0.045, or 0.075 mmol Fe/kg (n = 5) or placebo (n = 1). After intravenous injections, blood samples were collected for chemical and clinical analysis and relaxometry (0.94 T). Urinalyses were performed for up to 2 weeks after administration of the contrast medium.

None of the subjects showed significant abnormalities in safety laboratory parameters, and no serious adverse events were observed. Iron blood concentrations for all subjects showed no significant change (compared with baseline) after injection of VSOP-C184, for all subjects. However, plasma and serum iron concentrations increased significantly, reaching a peak level between 2 and 5 min post-injection, in correlation with the injected dose. The observed half-life was 0.5 to 1.5 h.

Results showed a reduction of T_1_ relaxation times of blood to <100 ms, for a time period of 17 ± 5 min after intravenous injection of VSOP-C184 at 0.045 mmol Fe/kg, and for 60 ± 9 min at 0.075 mmol Fe/kg. The values obtained for plasma were 68 ± 12 (0.045 mmol Fe/kg) and 148 ± 16 (0.075 mmol Fe/kg), respectively. Values obtained for serum were 59 ± 7 (0.045 mmol of Fe/kg) and 132 ± 21 (0.075 mmol Fe/kg). Some significant differences between the three dose groups were observed with respect to the minimum values of relaxation times T_1_ and T_2_ obtained for blood, plasma, and serum (p < 0.05). Ferritin levels were found to be normal both before and after injection of VSOP-C184, yet a dose-dependent increase was observed 2–8 days after administration of the contrast media at 0.045 and 0.075 mmol Fe/kg.

The results obtained in the study by Taupitz et al. (9) suggest that 0.015 mmol Fe/kg (the lowest of the three doses investigated) cannot produce an adequate effect for MRA in the equilibrium phase, whereas the highest dose, 0.075 mmol, causes overdose effects. A dose of about 0.045 mmol Fe/kg seems to be optimal for equilibrium MRA.

## References

1 Weissleder R, Hahn PF, Stark DD, Elizondo G, Saini S, Todd LE, Wittenberg J, Ferrucci JT. (1988). Superparamagnetic iron oxide: enhanced detection of focal splenic tumors with MR imaging. Radiology.
2 Kim SH, Choi D, Lim HK, Kim MJ, Jang KM, Kim SH, Lee WJ, Lee J, Jeon YH, Lim JH. (2006). Detection of hepatic VX2 carcinomas with ferucarbotran-enhanced magnetic resonance imaging in rabbits: Comparison of nine pulse sequences. Eur J Radiol.
3 Heesakkers RA, Futterer JJ, Hovels AM, van den Bosch HC, Scheenen TW, Hoogeveen YL, Barentsz JO. (2006). Prostate cancer evaluated with ferumoxtran-10-enhanced T2*-weighted MR Imaging at 1.5 and 3.0 T: early experience. Radiology.
4 Mutlu H, Basekim C, Silit E, Pekkafali Z, Ozturk E, Karaman B, Kantarci M, Kizilkaya E, Karsli F. (2006). Gadolinium-enhanced 3D MR angiography of pulmonary hypoplasia and aplasia. AJR Am J Roentgenol.
5 5. Terkivatan, T., I.C. van den Bos, S.M. Hussain, P.A. Wielopolski, R.A. de Man, J.N. Ijzermans, Focal nodular hyperplasia: Lesion characteristics on state-of-the-art MRI including dynamic gadolinium-enhanced and superparamagnetic iron-oxide-uptake sequences in a prospective study. J Magn Reson Imaging, 2006.
6 Kellar KE, Fujii DK, Gunther WH, Briley-Saebo K, Spiller M, Koenig SH. (1999). 'NC100150', a preparation of iron oxide nanoparticles ideal for positive-contrast MR angiography. MAGMA.
7 Allkemper T, Bremer C, Matuszewski L, Ebert W, Reimer P. (2002). Contrast-enhanced blood-pool MR angiography with optimized iron oxides: effect of size and dose on vascular contrast enhancement in rabbits. Radiology.
8 Wagner S, Schnorr J, Pilgrimm H, Hamm B, Taupitz M. (2002). Monomer-coated very small superparamagnetic iron oxide particles as contrast medium for magnetic resonance imaging: preclinical in vivo characterization. Invest Radiol.
9 Taupitz M, Wagner S, Schnorr J, Kravec I, Pilgrimm H, Bergmann-Fritsch H, Hamm B. (2004). Phase I clinical evaluation of citrate-coated monocrystalline very small superparamagnetic iron oxide particles as a new contrast medium for magnetic resonance imaging. Invest Radiol.
10 10. Pilgrimm, H., Superparamagnetic particles with increased R1 relaxivity, process for producing said particles and use thereof. EP 888545, JP 2000–507197.
11 Lawaczeck R, Bauer H, Frenzel T, Hasegawa M, Ito Y, Kito K, Miwa N, Tsutsui H, Vogler H, Weinmann HJ. (1997). Magnetic iron oxide particles coated with carboxydextran for parenteral administration and liver contrasting. Pre-clinical profile of SH U555A. Acta Radiol.
12 Weissleder R, Stark DD, Engelstad BL, Bacon BR, Compton CC, White DL, Jacobs P, Lewis J. (1989). Superparamagnetic iron oxide: pharmacokinetics and toxicity. AJR Am J Roentgenol.
13 Schnorr J, Wagner S, Abramjuk C, Wojner I, Schink T, Kroencke TJ, Schellenberger E, Hamm B, Pilgrimm H, Taupitz M. (2004). Comparison of the iron oxide-based blood-pool contrast medium VSOP-C184 with gadopentetate dimeglumine for first-pass magnetic resonance angiography of the aorta and renal arteries in pigs. Invest Radiol.
14 Schnorr J, Wagner S, Abramjuk C, Drees R, Schink T, Schellenberger EA, Pilgrimm H, Hamm B, Taupitz M. (2006). Focal Liver Lesions: SPIO-, Gadolinium-, and Ferucarbotran-enhanced Dynamic T1-weighted and Delayed T2-weighted MR Imaging in Rabbits. Radiology.